# ^66/67/68^Ga-γ-Deferoxamine-folate

Chemical name: | ^66/67/68^Ga-γ-Deferoxamine-folate
Abbreviated name: | ^66/67/68^Ga-γ-DF-folate
Synonym:
Agent category: | Folic acid (folate)
Target: | Putative folate receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET); single photon emission computed tomography (SPECT)
Source of signal: | ^66/67/68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=gallium%20deferoxamine%20folate)]

Folic acid (folate) is a water-soluble B vitamin (1) that is essential for methylation and DNA synthesis. The primary pathway for entry of folate into cells is through the facilitated transporter, which has a low affinity for folate (Michaelis constant (K_m_) = 1-5 μM). Some cells in the choroid plexus, kidney, lung, thyroid, spleen, placenta, and thymus also possess a higher affinity (dissociation constant (K_d_) = 0.5 nM) receptor that allows folate uptake via receptor-mediated endocytosis. Some human epithelial tumor cells were found to overexpress folate-binding protein (2). More than 90% of human ovarian and endometrial cancers express the high-affinity receptor, which is absent in normal tissues. Breast, colorectal, renal, and lung carcinomas also overexpress the folate receptor but at lower frequencies (20-50%). Activated macrophages, but not resting macrophages, have been also found to have folate receptor (3).

Several folate-based conjugates (^111^In-DTPA-folate, ^99m^Tc-EC-folate and [^18^F]FBA-folate) have been studied in tumor imaging (4-8). Deferoxamine (DF), a chelating agent, was conjugated to folic acid forming a mixture of two isomers, DF-α-folate and DF-γ-folate. Only the DF-γ-folate isomer was able to displace [^3^H]folic acid from its receptors with a similar IC_50_ to folic acid (2.5 versus 2.4 nM) (9). ^68/67/66^Ga-γ-DF-folate is being developed as an imaging agent for detection of folate receptors in vivo with either positron emission tomography (PET) or single photon emission computed tomography (SPECT).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=folate+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (folate receptor (http://www.ncbi.nlm.nih.gov/gene/2348))
- Articles in OMIM (folate receptor (http://www.ncbi.nlm.nih.gov/omim/136430))
- Clinical trials (folate receptors (http://www.clinicaltrials.gov/ct2/results?term=folate+receptor))
- Drug information in FDA (http://google2.fda.gov/search?q=folate+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=15)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=gallium%20deferoxamine%20folate%20and%20synthesis)]

Wang et al. (9) coupled DF-γ-folate (2.25 μmol) with 118 MBq (3.2 mCi) ^67^GA-(acetylacetone)_3_ in buffered saline at room temperature for 24 h to yield ^67^Ga-γ-DF-folate with >98% radiochemical purity. Radiochemical yields exceeded 80%. Mathias et al. (5) reported that ^66^Ga-γ-DF-folate and ^68^Ga-γ-DF-folate were similarly radiolabeled at 50°C for 15-30 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=gallium%20deferoxamine%20folate%20and%20in%20vitro)]

The human nasopharyngeal carcinoma KB-31 cell line has putative folate receptors as determined by [^3^H]folate binding studies in cultures (9). The mean IC_50_ values for DF-γ-folate, and folate were 25 and 24 nM, respectively. Binding of ^67^Ga-γ-DF-folate to cells was rapid and reached a maximal binding of 18% and 32% at 4°C and 37°C in 30 min, respectively. Both bindings were inhibited by folic acid and DF-γ-folate but not by DF-α-folate. As controls, ^67^Ga-DF and ^67^Ga-citrate showed little binding to the cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=gallium%20deferoxamine%20folate%20and%20rodentia)]

Mathias et al. (6, 10) performed biodistribution studies of ^67^Ga-γ-DF-folate in nude mice bearing the KB-31 tumor xenografts. The organ with the highest accumulation was the tumor (5.2%ID/g), followed by the kidneys (2.02%ID/g), and liver (0.46%ID/g) at 4 h after ^67^Ga-γ-DF-folate injection. Tumor/blood, tumor/muscle, tumor/liver and tumor/kidney ratio were 409, 124, 11, and 3, respectively. Pretreatment (5 min before the tracer) with folic acid (2.4 mg/mouse) reduced ^67^Ga-γ-DF-folate accumulation to 0.26%ID/g in the tumor. Administration of folate at 3.5 h after the tracer reduced the tumor accumulation to 2.22%ID/g at 4.5 h. ^67^Ga-DF showed no accumulation in the tumor.

The whole body distribution of ^66^Ga-γ-DF-folate (174 MBq or 4.7 mCi/mouse) was also assessed by PET imaging at 2.5 h after injection (5). The highest activity concentrations were visualized in the tumors and kidneys. The accumulation of ^66^Ga-γ-DF-folate in the tumors and kidneys was blocked by excess folic acid (0.9 mg/mouse) co-injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=gallium%20deferoxamine%20folate%20and%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=gallium%20deferoxamine%20folate%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=gallium%20deferoxamine%20folate%20and%20human)]

No publication is currently available.

## NIH Support

R01 CA86307, R01-CA70845

## References

1 Stanger O. (2002). Physiology of folic acid in health and disease. Curr Drug Metab.
2 Ke C.Y., Mathias C.J., Green M.A. (2003). The folate receptor as a molecular target for tumor-selective radionuclide delivery. Nucl Med Biol.
3 Nakashima-Matsushita N., Homma T., Yu S., Matsuda T., Sunahara N., Nakamura T., Tsukano M., Ratnam M., Matsuyama T. (1999). Selective expression of folate receptor beta and its possible role in methotrexate transport in synovial macrophages from patients with rheumatoid arthritis. Arthritis Rheum.
4 Mathias C.J., Hubers D., Low P.S., Green M.A. (2000). Synthesis of [(99m)Tc]DTPA-folate and its evaluation as a folate-receptor-targeted radiopharmaceutical. Bioconjug Chem.
5 Mathias C.J., Lewis M.R., Reichert D.E., Laforest R., Sharp T.L., Lewis J.S., Yang Z.F., Waters D.J., Snyder P.W., Low P.S., Welch M.J., Green M.A. (2003). Preparation of 66Ga- and 68Ga-labeled Ga(III)-deferoxamine-folate as potential folate-receptor-targeted PET radiopharmaceuticals. Nucl Med Biol.
6 Mathias C.J., Wang S., Low P.S., Waters D.J., Green M.A. (1999). Receptor-mediated targeting of 67Ga-deferoxamine-folate to folate-receptor-positive human KB tumor xenografts. Nucl Med Biol.
7 Mathias C.J., Wang S., Waters D.J., Turek J.J., Low P.S., Green M.A. (1998). Indium-111-DTPA-folate as a potential folate-receptor-targeted radiopharmaceutical. J Nucl Med.
8 Bettio A., Honer M., Muller C., Bruhlmeier M., Muller U., Schibli R., Groehn V., Schubiger A.P., Ametamey S.M. (2006). Synthesis and Preclinical Evaluation of a Folic Acid Derivative Labeled with 18F for PET Imaging of Folate Receptor-Positive Tumors. J Nucl Med.
9 Wang S., Lee R.J., Mathias C.J., Green M.A., Low P.S. (1996). Synthesis, purification, and tumor cell uptake of 67Ga-deferoxamine--folate, a potential radiopharmaceutical for tumor imaging. Bioconjug Chem.
10 Mathias C.J., Wang S., Lee R.J., Waters D.J., Low P.S., Green M.A. (1996). Tumor-selective radiopharmaceutical targeting via receptor-mediated endocytosis of gallium-67-deferoxamine-folate. J Nucl Med.